# ^89^Zr-N-Succinyldesferrioxamine-bevacizumab

Chemical name: | ^89^Zr-N-Succinyldesferrioxamine-bevacizumab
Abbreviated name: | ^89^Zr-Bevacizumab
Synonym:
Agent category: | Antibody
Target: | Vascular endothelial growth factor (VEGF)
Target category: | Antigen
Method of detection: | PET
Source of signal/contrast: | ^89^Zr
Activation: | No
Studies: | - Rodents | Click on protein (http://www.ncbi.nlm.nih.gov/entrez/viewer.fcgi?db=protein&val=71051581), nucleotide (http://www.ncbi.nlm.nih.gov/entrez/viewer.fcgi?val=NM_001025368.1) (RefSeq), and gene (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?db=gene&cmd=Retrieve&dopt=Graphics&list_uids=7422) for more information about VEGF.

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=Zirconium%20bevacizumab)]

Vascular endothelial growth factor (VEGF) consists of at least six isoforms of various numbers of amino acids (121, 145, 165, 183, 189, and 206 amino acids) produced through alternative splicing (1). VEGF_121_, VEGF_165_, and VEGF_189_ are the forms secreted by most cell types and are active as homodimers linked by disulfide bonds. VEGF_121_ does not bind to heparin like the other VEGF species do (2). VEGF is a potent angiogenic factor that induces proliferation, sprouting, migration, and tube formation of endothelial cells. There are three high-affinity tyrosine kinase VEGF receptors (VEGFR-1, Flt-1; VEGFR-2, KDR/Flt-1; and VEGFR-3, Flt-4) on endothelial cells. Several types of non-endothelial cells such as hematopoietic stem cells, melanoma cells, monocytes, osteoblasts, and pancreatic β cells also express VEGF receptors (1).

VEGF is overexpressed in various tumor cells and tumor-associated endothelial cells (3). Inhibition of VEGF receptor function has been shown to inhibit pathological angiogenesis as well as tumor growth and metastasis (4, 5). Radiolabeled VEGF has been developed as a single-photon emission computed tomography tracer for imaging solid tumors and angiogenesis in humans (6-8). However, several studies have shown that cancer treatments (photodynamic therapy, radiotherapy, and chemotherapy) can lead to increased tumor VEGF expression and subsequently to more aggressive disease (9, 10). Therefore, it is important to measure VEGF levels in the tumors to design better anti-cancer treatment protocols. Bevacizumab is a humanized antibody against VEGF-A. It binds to all VEGF isoforms. Bevacizumab is approved for clinical use in metastatic colon carcinoma and non-small cell lung cancer. Nagengast et al. (11) prepared ^89^Zr-N-succinyldesferrioxamine-bevacizumab (^89^Zr-bevacizumab) for imaging VEGF expression in nude mice bearing SKOV-3 human ovarian tumor xenografts.

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=Zirconium%20bevacizumab+synthesis)]

N-Succinyldesferrioxamine (N-sucDf) B-tetrafluorophenol and bevacizumab were incubated in sodium carbonate buffer (pH 9.5) for 30 min at room temperature (11). N-sucDf-Bevacizumab was isolated from the incubation mixture with ultrafiltration. There were 1.5–2.5 chelate groups per antibody. N-sucDf-Bevacizumab was mixed with ^89^Zr-oxalate. The mixture was incubated for 45 min at room temperature. ^89^Zr-Bevacizumab had a radiochemical purity of >99% and a specific activity 8.8 MBq/nmol (0.24 mCi/nmol) with a labeling yield of 98 ± 0.7%. ^89^Zr-Bevacizumab was stable for 7 d at 4°C in ammonium acetate and at 37°C in serum. ^89^Zr-Bevacizumab resulted in 54.0 ± 3.7% binding to VEGF. Bevacizumab (≥500-fold) almost completely blocked ^89^Zr-bevacizumab binding to <5%.

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=Zirconium%20bevacizumab+in+vitro)]

No publication is currently available.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=Zirconium%20bevacizumab+rodentia)]

Nagengast et al. (11) performed biodistribution studies of 3.5 MBq (0.095 mCi) ^89^Zr-bevacizumab (100 µg, ~0.66 nmol) in nude mice bearing human SKOV-3 ovarian tumor xenografts. Tumor uptake values were 4.85% injected dose (ID)/g at 1 d, 4.36% ID/g at 3 d, and 6.97% ID/g at 7 d. The radioactivity level in the blood was 9.54, 5.60, and 3.75% ID/g at 1, 3, and 7 d, respectively. The organs with the highest uptake were the lung (3.50% ID/g), liver (3.98% ID/g), spleen (3.22% ID/g), and kidneys (2.51% ID/g), with little radioactivity in the muscle (0.60% ID/g) at 3 d after injection. Tumor/muscle ratio was ~10. Tumor uptake determined with positron emission tomography images was 7.38 ± 2.06% ID/g for ^89^Zr-bevacizumab and 3.39 ± 1.16% ID/g for human ^89^Zr-IgG (P = 0.011) at 7 d. No blocking experiment was performed.

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=Zirconium%20bevacizumab+and+(dog+or+sheep+or+pig+or+rabbit))]

No publication is currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=Zirconium%20bevacizumab+and+(primate+not+human))]

No publication is currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=Zirconium%20bevacizumab+human)]

No publication is currently available.

## References

1 Ferrara N. (2004). Vascular endothelial growth factor: basic science and clinical progress. Endocr Rev.
2 Cohen T., Gitay-Goren H., Sharon R., Shibuya M., Halaban R., Levi B.Z., Neufeld G. (1995). VEGF121, a vascular endothelial growth factor (VEGF) isoform lacking heparin binding ability, requires cell-surface heparan sulfates for efficient binding to the VEGF receptors of human melanoma cells. J Biol Chem.
3 Soria J.C., Fayette J., Armand J.P. (2004). Molecular targeting: targeting angiogenesis in solid tumors. Ann Oncol.
4 Ferrara N. (2004). Vascular endothelial growth factor as a target for anticancer therapy. Oncologist.
5 Hicklin D.J., Ellis L.M. (2005). Role of the vascular endothelial growth factor pathway in tumor growth and angiogenesis. J Clin Oncol.
6 Li S., Peck-Radosavljevic M., Koller E., Koller F., Kaserer K., Kreil A., Kapiotis S., Hamwi A., Weich H.A., Valent P., Angelberger P., Dudczak R., Virgolini I. (2001). Characterization of (123)I-vascular endothelial growth factor-binding sites expressed on human tumour cells: possible implication for tumour scintigraphy. Int J Cancer.
7 Li S., Peck-Radosavljevic M., Kienast O., Preitfellner J., Hamilton G., Kurtaran A., Pirich C., Angelberger P., Dudczak R. (2003). Imaging gastrointestinal tumours using vascular endothelial growth factor-165 (VEGF165) receptor scintigraphy. Ann Oncol.
8 Li S., Peck-Radosavljevic M., Kienast O., Preitfellner J., Havlik E., Schima W., Traub-Weidinger T., Graf S., Beheshti M., Schmid M., Angelberger P., Dudczak R. (2004). Iodine-123-vascular endothelial growth factor-165 (123I-VEGF165). Biodistribution, safety and radiation dosimetry in patients with pancreatic carcinoma. Q J Nucl Med Mol Imaging.
9 Gorski D.H., Beckett M.A., Jaskowiak N.T., Calvin D.P., Mauceri H.J., Salloum R.M., Seetharam S., Koons A., Hari D.M., Kufe D.W., Weichselbaum R.R. (1999). Blockage of the vascular endothelial growth factor stress response increases the antitumor effects of ionizing radiation. Cancer Res.
10 Solban N., Selbo P.K., Sinha A.K., Chang S.K., Hasan T. (2006). Mechanistic investigation and implications of photodynamic therapy induction of vascular endothelial growth factor in prostate cancer. Cancer Res.
11 Nagengast W.B., de Vries E.G., Hospers G.A., Mulder N.H., de Jong J.R., Hollema H., Brouwers A.H., van Dongen G.A., Perk L.R., Lub-de Hooge M.N. (2007). In vivo VEGF imaging with radiolabeled bevacizumab in a human ovarian tumor xenograft. J Nucl Med.